# (E)-3-(Pyridin-2-ylethynyl)-cyclohex-2-enone-O-2-(2-[^18^F]fluoroethoxy)ethyl oxime

Chemical name: | (E)-3-(Pyridin-2-ylethynyl)-cyclohex-2-enone-O-2-(2-[^18^F]fluoroethoxy)ethyl-oxime
Abbreviated name: | [^18^F]FDEGPECO
Synonym:
Agent category: | Compound
Target: | Metabotropic glutamate receptor subtype 5 (mGluR5)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FDEGPECO)]

Glutamate is a major excitatory neurotransmitter at neuronal synapses in the central nervous system (CNS) (1). Glutamate produces its excitatory effects by acting on cell-surface ionotropic glutamate or metabotropic glutamate receptors (mGluRs). The mGluRs are GTP-binding-protein (G-protein)–coupled receptors that play important roles in regulating the activity of many synapses in the CNS, and many neuronal projection pathways contain mGluRs. There are eight mGluR subtypes. The fifth subtype, mGluR5, is usually found in postsynaptic neurons with moderate to high density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, and hippocampus, whereas the density in the cerebellum is low. The mGluR5 is positively coupled to phospholipase C in the regulation of neuronal excitability (2). Dysfunction of mGluR5 is implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal (3).

Positron emission tomography (PET) and single-photon emission tomography of radioligands targeting mGluR5 can visualize and analyze mGluR5 expression in normal physiological and pathological conditions. 2-Methyl-6-(phenylethynyl)-pyridine (MPEP) and its methyl analog M-MPEP have been identified as potent, highly selective, noncompetitive antagonists for mGluR5. These mGluR5 antagonists have been successfully labeled, but their impact as targeted imaging agents has been limited by high lipophilicity, lack of mGluR subtype selectivity, and unfavorable brain accumulation kinetics (3, 4). Based on the structure of MPEP, 3-(6-methyl-pyridin-2-ylethynyl)-cyclohex-2-enone-O-[^11^C]-methyl-oxime ([^11^C]ABP688) was synthesized and evaluated as a potential PET imaging agent for mGluR5; this agent produced strong and specific signals in rodent and human brain tissue (5-8). Using ABP688 as a template, 3-(pyridin-2-ylethynyl)-cyclohex-2-enone-O-[^18^F]fluoroethyl-oxime ([^18^F]fluoroethyl-desmethyl-ABP688 or [^18^F]FE-DABP688) was synthesized and evaluated as a specific PET imaging tool for mGluR5 (9). Wanger-Baumann et al. (10) have developed a new DABP688 derivative, (E)-3-(pyridin-2-ylethynyl)-cyclohex-2-enone-O-2-(2-[^18^F]fluoroethoxy)ethyl-oxime ([^18^F]FDEGPECO), for use with in vivo PET imaging of mGluR5.

### Related Resource Links:

- Chapters in MICAD (mGluR5 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=mGluR5+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (mGluR5 (http://www.ncbi.nlm.nih.gov/gene/2915))
- Articles in OMIM (mGluR5 (http://www.ncbi.nlm.nih.gov/omim/604102))
- Clinical trials (mGluR5 (http://www.clinicaltrials.gov/ct2/results?term=mglur5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDEGPECO%20and%20synthesis)]

Wanger-Baumann et al. (10) reported a one-step synthesis of [^18^F]FDEGPECO. The tosyl-precursor was subjected to nucleophilic fluorination with K[^18^F]F/Kryptofix2.2.2 for 10 min at 90°C, with a radiochemical yield of 40% and a specific activity of 80–320 GBq/μmol (2.1–8.6 Ci/μmol) after purification with high-performance liquid chromatography. The total synthesis time was 45 min. The radiochemical purity of [^18^F]FDEGPECO was >98%. [^18^F]FDEGPECO exhibited a log D_7.4_ value of 1.7 ± 0.1. [^18^F]FDEGPECO was stable for up to 120 min in human and rat plasma and in vitro at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDEGPECO%20and%20in%20vitro)]

In vitro binding of [^18^F]FDEGPECO was studied in rat brain tissue membranes (11). Saturation studies indicated that the receptor binding was saturable, and Scatchard plot analysis indicated two affinity binding sites with dissociation constants of 0.6 ± 0.2 nM and 13.7 ± 4.7 nM (n = 3). In vitro autoradiography showed that [^18^F]FDEGPECO bound heterogeneously to the brain sections, with the highest accumulation of radioactivity in the mGluR-rich hippocampus, striatum, and cingulate cortex and with low radioactivity in the cerebellum (10). Co-incubation with excess ABP688 reduced the level of accumulated radioactivity to that of the cerebellum.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDEGPECO%20and%20rodentia)]

Wanger-Baumann et al. (10) performed ex vivo biodistribution studies in six normal rats that received intravenous injections of 8–16 MBq (0.22–0.43 mCi) [^18^F]FDEGPECO. Results at 15 min after injection (the only time point studied) showed that the highest radioactivity concentrations (expressed as percent of injected dose/gram (% ID/g)) were observed in mGluR5-rich brain regions such as the hippocampus (0.17 ± 0.02% ID/g) and striatum (0.20 ± 0.03% ID/g), whereas radioactivity accumulation was lowest in the cerebellum (0.06 ± 0.006% ID/g). The hippocampus/cerebellum and striatum/cerebellum ratios were 2.8 and 3.3, respectively. Co-injection of 1 mg/kg M-MPEP, a specific ligand for mGluR5, with [^18^F]FDEGPECO decreased the accumulation of radioactivity by 54% and 50% in the hippocampus and striatum, respectively. Little inhibition was observed in the cerebellum. The peripheral organ with the highest accumulation was the liver (0.37% ID/g), followed by the kidney, bone, lung, blood, and muscle, which each had radioactivity levels of <0.11% ID/g. [^18^F]FDEGPECO was 91% and 75% intact in the brain and plasma, respectively, at 17 min after injection. Only one radiometabolite, which was more hydrophilic, was detected in the plasma.

PET imaging over 40-60 min in rats showed the highest radioactivity levels in the intestines and liver. The hippocampus, striatum, and cingulate showed high radioactivity as compared to the cerebellum. Co-injection of 1 mg/kg M-MPEP reduced the accumulation in the hippocampus, striatum, and cingulate to that in the cerebellum. Equilibrium between specific and background activity was reached in 15-20 min.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDEGPECO%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDEGPECO%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDEGPECO%20and%20human)]

No publication is currently available.

## References

1 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
2 Abe T., Sugihara H., Nawa H., Shigemoto R., Mizuno N., Nakanishi S. (1992). Molecular characterization of a novel metabotropic glutamate receptor mGluR5 coupled to inositol phosphate/Ca2+ signal transduction. J Biol Chem.
3 Gasparini F., Lingenhohl K., Stoehr N., Flor P.J., Heinrich M., Vranesic I., Biollaz M., Allgeier H., Heckendorn R., Urwyler S., Varney M.A., Johnson E.C., Hess S.D., Rao S.P., Sacaan A.I., Santori E.M., Velicelebi G., Kuhn R. (1999). 2-Methyl-6-(phenylethynyl)-pyridine (MPEP), a potent, selective and systemically active mGlu5 receptor antagonist. Neuropharmacology.
4 Yu M., Tueckmantel W., Wang X., Zhu A., Kozikowski A.P., Brownell A.L. (2005). Methoxyphenylethynyl, methoxypyridylethynyl and phenylethynyl derivatives of pyridine: synthesis, radiolabeling and evaluation of new PET ligands for metabotropic glutamate subtype 5 receptors. Nucl Med Biol.
5 Ametamey S.M., Kessler L.J., Honer M., Wyss M.T., Buck A., Hintermann S., Auberson Y.P., Gasparini F., Schubiger P.A. (2006). Radiosynthesis and preclinical evaluation of 11C-ABP688 as a probe for imaging the metabotropic glutamate receptor subtype 5. J Nucl Med.
6 Ametamey S.M., Treyer V., Streffer J., Wyss M.T., Schmidt M., Blagoev M., Hintermann S., Auberson Y., Gasparini F., Fischer U.C., Buck A. (2007). Human PET studies of metabotropic glutamate receptor subtype 5 with 11C-ABP688. J Nucl Med.
7 Hintermann S., Vranesic I., Allgeier H., Brulisauer A., Hoyer D., Lemaire M., Moenius T., Urwyler S., Whitebread S., Gasparini F., Auberson Y.P. (2007). ABP688, a novel selective and high affinity ligand for the labeling of mGlu5 receptors: identification, in vitro pharmacology, pharmacokinetic and biodistribution studies. Bioorg Med Chem.
8 Wyss M.T., Ametamey S.M., Treyer V., Bettio A., Blagoev M., Kessler L.J., Burger C., Weber B., Schmidt M., Gasparini F., Buck A. (2007). Quantitative evaluation of 11C-ABP688 as PET ligand for the measurement of the metabotropic glutamate receptor subtype 5 using autoradiographic studies and a beta-scintillator. Neuroimage.
9 Honer M., Stoffel A., Kessler L.J., Schubiger P.A., Ametamey S.M. (2007). Radiolabeling and in vitro and in vivo evaluation of [(18)F]-FE-DABP688 as a PET radioligand for the metabotropic glutamate receptor subtype 5. Nucl Med Biol.
10 Wanger-Baumann C.A., Mu L., Honer M., Belli S., Alf M.F., Schubiger P.A., Kramer S.D., Ametamey S.M. (2011). In vitro and in vivo evaluation of [18F]-FDEGPECO as a PET tracer for imaging the metabotropic glutamate receptor subtype 5 (mGluR5). Neuroimage.
11 Baumann C.A., Mu L., Johannsen S., Honer M., Schubiger P.A., Ametamey S.M. (2010). Structure-activity relationships of fluorinated (E)-3-((6-methylpyridin-2-yl)ethynyl)cyclohex-2-enone-O-methyloxime (ABP688) derivatives and the discovery of a high affinity analogue as a potential candidate for imaging metabotropic glutamate recepors subtype 5 (mGluR5) with positron emission tomography (PET). J Med Chem.